# ^64^Cu-1,4,8,11-Tetraazacyclotetradecane-N,N',N",N"'-tetraacetic acid-D-Phe-cyclo(Cys-Tyr-D-Trp-Lys-Thr-Cys)-Thr(OH)

Chemical name: | ^64^Cu-1,4,8,11-Tetraazacyclotetradecane-N,N',N",N"'-tetraacetic acid-D-Phe-cyclo(Cys-Tyr-D-Trp-Lys-Thr-Cys)-Thr(OH)
Abbreviated name: | ^64^Cu-TETA-Y3-TATE
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor (sst_2_)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human Primates | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (sst_1_–sst_5_) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Labeled diethylenetriaminepentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SSTR analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). OCT is a cyclic peptide with eight amino acids. ^111^In-DTPA-OCT binds with high affinity to SSTR subtypes 2 and 5 (sst_2_ and sst_5_) and to sst_3_ to a lesser degree, but it does not bind to sst_1_ or sst_4_ (8). Currently used targeting SSTR peptides mainly have sst_2_ affinity for sst_2_. D-Phe-cyclo(Cys-Tyr-D-Trp-Lys-Thr-Cys)-Thr(OH) ([Tyr3]-octreotate (Y3-TATE)) was found to be a selective sst_2_ agonist (9). For evaluation as a positron emission tomography (PET) imaging agent for sst_2_, ^64^Cu has been attached to Y3-TATE via 1,4,8,11-tetraazacyclotetradecane-N,N',N",N"'-tetraacetic acid (TETA) to form ^64^Cu-TETA-Y3-TATE (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+synthesis)]

TETA-Y3-TATE was synthesized with standard solid-phase peptide synthesis (10). TETA-Y3-TATE was purified with high-performance liquid chromatography with a confirmed molecular weight of 1,050 Da as measured with mass spectroscopy. ^64^Cu was complexed to TETA-Y3-TATE by reaction of 0.6–6.0 nmol TETA-Y3-TATE with 37–185 MBq (1–5 mCi) ^64^CuCl_2_ in 0.1 M ammonium acetate (pH 5.5) for 1 h at 37°C. ^64^Cu-TETA-Y3-TATE had a >98% radiochemical purity and specific activity of 30–108 GBq/µmol (0.8–2.9 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+in+vitro)]

Lewis et al. (10) determined that ^64^Cu-TETA-Y3-TATE showed a K_d_ (affinity constant) of 0.55 nM and a B_max_ (receptor density) of 0.12 pmol/mg protein in CA20948 rat pancreatic tumor cell membranes. Reubi et al. (9) reported that DTPA-Y3-TATE had 50% inhibition concentration (IC_50_) values of >1,000, 3.9 ± 1.0, >1,000, >1,000, and >1,000 nM for human sst_1_, sst_2_, sst_3_, sst_4_, and sst_5_ receptors in competition with ^125^I-SRIF-28, respectively. ^64^Cu-TETA-Y3-TATE was internalized into AR42J tumor cells in culture, and the internalization was blocked by excess Y3-TATE (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+rodentia)]

Lewis et al. (10) performed ex vivo biodistribution studies with ^64^Cu-TETA-Y3-TATE in rats (n = 5/group) bearing xenografts of CA20948 tumors at 1, 4, and 24 h after injection. The accumulation of radioactivity in the sst_2_ tumors was 2.4% injected dose per gram (% ID/g) at 1 h, 2.2% ID/g at 4 h, and 0.6% ID/g at 24 h after injection. The adrenal and pancreas had the highest accumulation at 1 h after injection (~9% ID/g each), followed by the kidney (1.5% ID/g) and bone (0.5% ID/g). The concentration in the blood and muscle was <0.1% ID/g, with a tumor/blood ratio of 28 and a tumor/muscle ratio of 140 at 4 h after injection. Co-injection with Y3-TATE reduced the accumulation of radioactivity by >90% in the tumors, adrenal, and pancreas, as well as ~80% inhibition in the bone at 1 h after injection. Little or no inhibition was observed in the other tissues tested.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+(primate+not+human))]

Whole-body PET imaging of a male baboon visualized the pituitary, kidneys, liver, and urinary bladder at 1 h after injection of ^64^Cu-TETA-Y3-TATE (10). Little radioactivity was observed in the lung and bone.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Y3-TATE+and+human)]

No publication is currently available.

## NIH Support

R01 CA064475, R01 EB004533, R24 CA86307

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
10 Lewis J.S., Srinivasan A., Schmidt M.A., Anderson C.J. (1999). In vitro and in vivo evaluation of 64Cu-TETA-Tyr3-octreotate. A new somatostatin analog with improved target tissue uptake. Nucl Med Biol.
11 Sprague J.E., Peng Y., Sun X., Weisman G.R., Wong E.H., Achilefu S., Anderson C.J. (2004). Preparation and biological evaluation of copper-64-labeled tyr3-octreotate using a cross-bridged macrocyclic chelator. Clin Cancer Res.